# ^64^Cu-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-conatumumab

Chemical name: | ^64^Cu-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-conatumumab
Abbreviated name: | ^64^Cu-DOTA-conatumumab
Synonym: | ^64^Cu-DOTA-AMG 655
Agent category: | Antibody
Target: | Death receptor 5 (DR5), also known as TRAIL-R2 (TR2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=conatumumab)]

The tumor necrosis factor–related apoptosis-inducing ligand (TRAIL) receptor is a member of the tumor necrosis factor superfamily of cytokines that selectively activate a complex apoptotic pathway (caspase cascade) in tumor cells, thereby inducing apoptosis (cell death) (1, 2). There are two cell-surface TRAIL receptors (death receptor 4 [DR4] and 5 [DR5]) that are capable of inducing apoptosis and three decoy TRAIL receptors that are not capable of inducing apoptotic signals (3, 4). Conatumumab is a fully human monoclonal antibody (mAb) that acts as a human DR5 agonist antibody to tumor cells, which causes apoptosis in in vitro and in vivo studies (5, 6). Conatumumab is being evaluated in clinical trials (7, 8). Rossin et al. (9) reported the development of ^64^Cu-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-conatumumab (^64^Cu-DOTA-conatumumab) for positron emission tomography (PET) imaging of DR5 in nude mice bearing tumor xenografts.

### Related Resource Links:

- Chapters in MICAD (DR5 (http://www.ncbi.nlm.nih.gov/books?term=trail%20receptor%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (DR5 (http://www.ncbi.nlm.nih.gov/gene/8795))
- Articles in Online Mendelian Inheritance in Man (OMIM) (DR5 (http://omim.org/entry/603612?search=dr5&highlight=dr5))
- Clinical trials (Conatumumab (http://www.clinicaltrials.gov/ct2/results?term=conatumumab))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20conatumumab+synthesis)]

2,2',2''-(10-(2-(2,5-dioxopyrrolidin-1-yloxy)-2-oxoethyl)-1,4,7,10-tetraazacyclododecane-1,4,7-triyl)triacetic acid (DOTA-N-hydroxysuccinimide) was added to conatumumab (100 nmol) in phosphate-buffered saline (9). The reaction mixture was adjusted to pH 8.5 and incubated for ~2 h at room temperature. DOTA-conatumumab was purified with column chromatography. DOTA-conatumumab (0.6–1.2 nmol) was incubated with 33–222 MBq (1–6 mCi) ^64^CuCl_2_ in ammonium acetate buffer (pH 5.5) for 1 h at 37°C. ^64^Cu-DOTA-conatumumab was purified with column chromatography, with a radiochemical purity of >95%. The specific activities were 6 MBq/nmol (0.16 mCi/nmol) and 123 MBq/nmol (3.3 mCi/nmol) for ex vivo biodistribution studies and PET studies, respectively. There were approximately five DOTA molecules per antibody. ^64^Cu-DOTA-conatumumab was stable in mouse serum for 24 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20conatumumab%20in+vitro)]

Rossin et al. (9) performed competition binding experiments using a conatumumab immobilized Biacore sensor chip. DOTA-conatumumab and conatumumab inhibited the binding of huTR2-Fc (1 nM) with 50% inhibition concentration (IC_50_) values of 0.389 nM and 0.320 nM, respectively. The potency of DOTA-conatumumab and conatumumab to induce caspase 3/7 activities was compared in Colo205 human colon tumor cells. The effective doses to induce 50% of the maximum caspase 3/7 activities were 0.135 ± 0.31 nM and 0.128 ± 0.30 nM (n = 5), respectively. These data suggest that DOTA-conatumumab and conatumumab exhibit similar immunoreactivity and agonist activity for DR5.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20conatumumab+rodentia)]

Rossin et al. (9) performed PET and ex vivo biodistribution studies of 0.33 MBq (0.009 mCi) ^64^Cu-DOTA-conatumumab (52 pmol) in nude mice (n = 4/group) bearing Colo205 tumors at 6 h and 24 h after injection. Ex vivo tumor accumulation values were 13.86 ± 1.19% injected dose/gram (ID/g) and 20.68 ± 3.03% ID/g at 6 h and 24 h after injection, respectively. Accumulation at 24 h after injection was highest in the spleen (42.66% ID/g), followed by the blood (18.14% ID/g), liver (10.75% ID/g), lung (9.30% ID/g), heart (6.06% ID/g), and kidney (5.99% ID/g). Co-injection of conatumumab (2 nmol) decreased the radioactivity levels in the tumors and spleen by 50%–60% at 6 h and 24 h after injection. The binding in the spleen may be because of binding of ^64^Cu-DOTA-conatumumab to splenic Fc receptors on macrophages. Little inhibition was observed in the other normal tissues. ^64^Cu-DOTA-conatumumab remained >98% intact in the blood at 24 h after injection.

Whole-body PET images were obtained in the tumor-bearing mice (n = 2/group) at 1, 6 and 24 h after injection of 3.7 MBq (0.1 mCi) ^64^Cu-DOTA-conatumumab (30 pmol) (9). High levels of background radioactivity were detected at 1 h and 6 h. However, the tumors could be visualized at 6 h. The standard uptake value (SUV) of the tumors was 3.16 at 24 h. Co-injection of conatumumab (2 nmol) decreased the SUV to 1.55 with ~50% inhibition. The spleen SUV decreased from 1.73 (control) to 1.23 (blocked).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20conatumumab+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20conatumumab+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu%20conatumumab+human)]

No publication is currently available.

## NIH Support

CA86307

## References

1 Wang S. (2010). TRAIL: a sword for killing tumors. Curr Med Chem.
2 Fox N.L., et al. (2010). Tumor Necrosis Factor-related apoptosis-inducing ligand (TRAIL) Receptor-1 and Receptor-2 agonists for cancer therapy. Expert Opin Biol Ther.
3 Ashkenazi A., Dixit V.M. (1999). Apoptosis control by death and decoy receptors. Curr Opin Cell Biol.
4 Spierings D.C., et al. (2004). Tissue distribution of the death ligand TRAIL and its receptors. J Histochem Cytochem.
5 Rosevear H.M., Lightfoot A.J., Griffith T.S. (2010). Conatumumab, a fully human mAb against death receptor 5 for the treatment of cancer. Curr Opin Investig Drugs.
6 Kaplan-Lefko P.J., et al. (2010). Conatumumab, a fully human agonist antibody to death receptor 5, induces apoptosis via caspase activation in multiple tumor types. Cancer Biol Ther.
7 Wiezorek J., Holland P., Graves J. (2010). Death receptor agonists as a targeted therapy for cancer. Clin Cancer Res.
8 Soria J.C., et al. (2010). Phase 1b study of dulanermin (recombinant human Apo2L/TRAIL) in combination with paclitaxel, carboplatin, and bevacizumab in patients with advanced non-squamous non-small-cell lung cancer. J Clin Oncol.
9 Rossin R., et al. (2011). Characterization of 64Cu-DOTA-conatumumab: a PET tracer for in vivo imaging of death receptor 5. J Nucl Med.